# Gadolinium-1,4,7,10-tetraazacyclododecane-N',N'',N''',N''''-tetraacetic acid-Pro-Leu-Ala-Leu-Lys-Arg-Asp-Arg

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-N',N'',N''',N''''-tetraacetic acid-Pro-Leu-Ala-Leu-Lys-Arg-Asp-Arg
Abbreviated name: | Gd-DOTA-PCA7
Synonym: | Gd-DOTA-PCA7-switch
Agent Category: | Peptide
Target: | Matrix metalloproteinase-7 (MMP-7)
Target Category: | Enzyme binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=13177712), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=75709180) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4316&ordinalpos=2&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about MMP-7.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA7)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1).

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (2). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (3). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degradation of the basement membrane and ECM (4). Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (5-8). MMP-7, also known as matrilysin, is frequently overexpressed in human cancer tissues and is associated with cancer progression (9, 10). MMP-7 has been shown to play important roles not only in degradation of ECM proteins but also in the regulation of activation, degradation, and shedding of non-ECM proteins (11).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (12, 13). Gd-Labeled diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Various macromolecular Gd complexes have demonstrated superior contrast enhancement for MRI of the vasculature and carcinomas (14-16); however, these Gd complexes cannot proceed into further clinical development because of high tissue accumulation and slow excretion of toxic Gd ions. Furthermore, they are largely nonspecific. An MMP-7 selective peptide, Pro-Leu-Ala-Leu-Lys-Arg-Asp-Arg (PLALKRDR), was found to be selectively cleaved by MMP-7 (17). Proteinase-modulated contrast agents (PCAs) are used with MRI to detect the activity of proteinases in vivo. The PCAs are based on the concept of a solubility switch, from hydrophilic to hydrophobic, which slows their efflux from the activity site. Gd-1,4,7,10-tetraazacyclododecane-N',N'',N''',N''''-tetraacetic acid-PLALKRDR (Gd-DOTA-PCA7-switch) was developed to detect MMP-7 activity in tumor-bearing mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA7+synthesis)]

PCA7-switch, prepared with solid-phase synthesis, was coupled to DOTA with the use of DOTA-tri(t-butyl ester) (17). DOTA-PCA7-switch was isolated with column chromatography and incubated with 1.05-molar equivalents of GdCl_3_ for 24 h. Gd-DOTA-PCA7-switch was purified with high-performance liquid chromatography (HPLC) with a 61% yield. The mass of Gd-DOTA-PCA7-switch was confirmed with mass spectroscopy. Two control Gd-DOTA-PCAs were also prepared: PCA7-scrambled with an MMP-7–resistant peptide (RAKDRLLP), and PCA7-B with hydrophobic proteolytic cleavage products.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA7+in+vitro)]

PCA7-switch formed a more hydrophobic product after incubation in the presence of MMP-7 as determined with HPLC analysis (17). There was no change in T1 relaxation times and only 10% change in T2 relaxation times for PCA7-switch after MMP-7 cleavage. On the other hand, PCA7-B showed little difference in hydrophobicity as well as 35% change in T1 relaxation times and 75% change in T2 relaxation times after MMP-7 cleavage, possibly through aggregation after cleavage.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA7+rodentia)]

Lepage et al. (17) used a 7-T MRI animal scanner to perform in vivo MRI in mice (n = 5) bearing human SW480 (MMP-7–negative) and SW480Mat (MMP-7–positive) colon cancer cells on the left and right hind limbs, respectively. Injection of Gd-DOTA-PCA7-switch (3.7 µmol/mouse) provided a steady enhancement in MRI contrast in the core of SW480Mat tumors within 60 min of injection, which continued up to 160 min. The rim of the tumor showed a marked clearance. All five mice injected with Gd-DOTA-PCA7-switch exhibited a significant difference in signal intensity between the MMP-7–positive and MMP-7–negative tumors (P < 0.01). On the other hand, the core of SW480 tumors showed a gradual decline in signal intensity after 60 min. Mice tested with Gd-DOTA-PCA7-scramble (2.3 µmol/mouse) and Gd-DTPA (10 µmol/mouse) showed much less pronounced differences between the two tumors. Pretreatment with GM6001 MMP-7 inhibitor (100 mg/kg per d) for 3 d in the mice bearing two tumors eliminated the difference in signal intensity between the two tumors by inhibiting the accumulation of the signal in the MMP-7–positive tumor. The washout was also faster in the MMP-7–positive tumors after GM6001 treatment.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA7+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA7+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA7+human)]

No publication is currently available.

## NIH Support

P30 CA068485, R41 RR020835

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
3 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
4 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
5 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
6 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
7 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
8. Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007.
9 Shiomi T., Okada Y. (2003). MT1-MMP and MMP-7 in invasion and metastasis of human cancers. Cancer Metastasis Rev.
10 Zucker S., Vacirca J. (2004). Role of matrix metalloproteinases (MMPs) in colorectal cancer. Cancer Metastasis Rev.
11 Ii M., Yamamoto H., Adachi Y., Maruyama Y., Shinomura Y. (2006). Role of matrix metalloproteinase-7 (matrilysin) in human cancer invasion, apoptosis, growth, and angiogenesis. Exp Biol Med (Maywood).
12 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
13 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
14 Schmiedl U., Ogan M., Paajanen H., Marotti M., Crooks L.E., Brito A.C., Brasch R.C. (1987). Albumin labeled with Gd-DTPA as an intravascular, blood pool-enhancing agent for MR imaging: biodistribution and imaging studies. Radiology.
15 Gossmann A., Okuhata Y., Shames D.M., Helbich T.H., Roberts T.P., Wendland M.F., Huber S., Brasch R.C. (1999). Prostate cancer tumor grade differentiation with dynamic contrast-enhanced MR imaging in the rat: comparison of macromolecular and small-molecular contrast media--preliminary experience. Radiology.
16 Preda A., van Vliet M., Krestin G.P., Brasch R.C., van Dijke C.F. (2006). Magnetic resonance macromolecular agents for monitoring tumor microvessels and angiogenesis inhibition. Invest Radiol.
17 Lepage M., Dow W.C., Melchior M., You Y., Fingleton B., Quarles C.C., Pepin C., Gore J.C., Matrisian L.M., McIntyre J.O. (2007). Noninvasive detection of matrix metalloproteinase activity in vivo using a novel magnetic resonance imaging contrast agent with a solubility switch. Mol Imaging.